# Cy5.5-Ferritin nanocages

Chemical name: | Cy5.5-Ferritin nanocages
Abbreviated name: | Cy5.5-Fn nanocages
Synonym:
Agent category: | Polypeptide nanoparticle
Target: | Non-targeted
Target category: | Non-targeted
Method of detection: | Optical, near-infrared (NIR) fluorescence
Source of signal: | Cy5.5
Activation: | No
Studies: | - In vitro; - Rodents | Structure is not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Ferritin%20nanoparticle)]

Optical fluorescence imaging is increasingly used to monitor biological functions of specific targets in small animals (1-3). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–700 nm) are used. Near-infrared (NIR) fluorescence (700–1,000 nm) detection avoids the background fluorescence interference of natural biomolecules, providing a high contrast between target and background tissues. NIR fluorophores have a wider dynamic range and minimal background as a result of reduced scattering compared with visible fluorescence detection. They also have high sensitivity, resulting from low fluorescence background, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence (NIRF) imaging is becoming a noninvasive alternative to radionuclide imaging in small animals (4).

Endothelial cells are important cells in inflammatory responses (5, 6). Bacterial lipopolysaccharides, viruses, inflammation, and tissue injury increase secretion of tumor necrosis factor α (TNFα), interleukin-1 (IL-1), and other cytokines and chemokines. Emigration of leukocytes from blood is dependent on their ability to adhere to endothelial cell surfaces. Inflammatory mediators and cytokines induce chemokine secretion from endothelial cells and other vascular cells and increase their expression of cell-surface adhesion molecules, such as intracellular adhesion molecule-1, vascular cell adhesion molecule-1, integrins, and selectins. Chemokines are chemotactic to inflammatory cells (leukocytes and macrophages) attracting them to sites of inflammation and tissue injury. Under atherogenic conditions, deposition of lipids on the endothelial cell surfaces of the aorta and inflammatory cells leads to the development of atherosclerotic plaques (7), which may erode and rupture.

Ferritin (Fn) is composed of 24 subunits of heavy and light chains, which self-assemble to form a cagelike nanoparticle (nanocage) at physiological pH (7.4) with internal and external diameters of 8 nm and 12 nm (8, 9), respectively. The outer surface of Fn can be chemically or genetically modified with ligands, and the cavity of Fn can capture metal ions with high affinity (10). Terashima et al. (11) chemically coupled Cy5.5 onto human heavy chain Fn (Cy5.5-Fn) nanocages. Cy5.5-Fn nanocages have been studied for NIRF imaging of vascular macrophages in atherosclerotic plaques in mice.

### Related Resource Links:

- Chapters in MICAD (Ferritin (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=Ferritin+AND+micad%5Bbook%5D))
- Gene information in NCBI (Ferritin heavy chain (http://www.ncbi.nlm.nih.gov/gene/2495), ferritin light chain (http://www.ncbi.nlm.nih.gov/gene/2512))
- Articles in Online Mendelian Inheritance in Man (OMIM) (Ferritin heavy chain (http://www.ncbi.nlm.nih.gov/omim/134770), ferritin light chain (http://www.ncbi.nlm.nih.gov/omim/134790))
- Clinical trials (Ferritin (http://www.clinicaltrials.gov/ct2/results?term=ferritin))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Ferritin%20nanoparticle+synthesis)]

Recombinant human Fn subunits were purified from transfected Escherichia coli cell lysates. Cy5.5-Fn was prepared by incubation of Cy5.5-NHS ester with Fn (pH 8.2) for 1 h at room temperature, followed by overnight incubation at 4°C. Cy5.5-Fn was isolated with column chromatography (11). There were four Cy5.5 molecules per Fn nanocage.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Ferritin%20nanoparticle+in%20vitro)]

The external diameters of Cy5.5-Fn nanocages and unlabeled Fn-nanocages were determined to be ~12 nm with transmission electron microscopy at pH 7.4 (11).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Ferritin%20nanoparticle+rodentia)]

Terashima et al. (11) performed NIRF imaging of macrophages in atherosclerotic carotid arteries in streptozotocin (STZ)-induced diabetic mice. At day 14 after STZ injection, the left common carotid artery (LCA) was ligated in 11 mice and sham-operated in 3 mice. Cy5.5-Fn nanocages (8 nmol Cy5.5) were injected intravenously via retro-orbital injection. NIRF images of both LCA and right common carotid artery (RCA) were obtained at 48 h after injection. There was a clear signal localized to the macrophage-rich ligated LCA, but not to the control RCA or to either artery in sham-operated mice. Quantitative analysis showed that the NIRF signal was significantly higher in the ligated LCA compared to the contralateral RCA and sham controls (P < 0.04). Ex vivo NIRF images of the arteries confirmed the findings with in vivo NIRF imaging (P < 0.002). Immunohistochemical analysis showed macrophage infiltration in the ligated LCA but not in the non-ligated RCA. Cy5.5-Fn was co-localized with macrophages in the LCA. However, no blocking studies were reported, but permeability differences between ligated LCA and control have been reported

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Ferritin%20nanoparticle+and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Ferritin%20nanoparticle+and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Ferritin%20nanoparticle+human)]

No publication is currently available.

## NIH Support

R01 HL078678, R21 EB005364

## References

1 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
2 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
3 Becker A., Hessenius C., Licha K., Ebert B., Sukowski U., Semmler W., Wiedenmann B., Grotzinger C. (2001). Receptor-targeted optical imaging of tumors with near-infrared fluorescent ligands. Nat Biotechnol.
4 Tung C.H. (2004). Fluorescent peptide probes for in vivo diagnostic imaging. Biopolymers.
5 Cybulsky M.I., Gimbrone M.A. (1991). Endothelial expression of a mononuclear leukocyte adhesion molecule during atherogenesis. Science.
6 Lowe J.B. (2002). Glycosylation in the control of selectin counter-receptor structure and function. Immunol Rev.
7 Libby P. (2002). Inflammation in atherosclerosis. Nature.
8 Maham A., Tang Z., Wu H., Wang J., Lin Y. (2009). Protein-based nanomedicine platforms for drug delivery. Small.
9 Uchida M., Kang S., Reichhardt C., Harlen K., Douglas T. (2010). The ferritin superfamily: Supramolecular templates for materials synthesis. Biochim Biophys Acta.
10 Uchida M., Flenniken M.L., Allen M., Willits D.A., Crowley B.E., Brumfield S., Willis A.F., Jackiw L., Jutila M., Young M.J., Douglas T. (2006). Targeting of cancer cells with ferrimagnetic ferritin cage nanoparticles. J Am Chem Soc.
11 Terashima M., Uchida M., Kosuge H., Tsao P.S., Young M.J., Conolly S.M., Douglas T., McConnell M.V. (2011). Human ferritin cages for imaging vascular macrophages. Biomaterials.